# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-1,4,7,10-tetraacetic acid-rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-1,4,7,10-tetraacetic acid-rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_
Abbreviated name: | ^64^Cu-DOTA-ReCCMSH(Arg^11^)
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 (MC-1) receptor, MC1R
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the Melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH)]

Malignant melanoma is the most deadly form of skin cancer (1). Early and accurate diagnosis is necessary for surgery and successful treatment (2). The melanocortin (MC) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (3). Most cutaneous cell types express MC receptors, pro-opiomelanocortin (POMC), and prohormone convertases, and they also release MCs. Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily. However, these receptors have been found to be overexpressed in melanoma cells (4, 5). α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (6) in the regulation of skin pigmentation via the MC1R.

Although positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (7, 8). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R that is overexpressed on human and mouse melanoma cells (4, 5, 7, 9, 10). 1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) has been successfully coupled to the α-MSH peptide analogs for radiolabeling with a variety of radionuclides (7). ^111^In- and ^99m^Tc-DOTA-Re(Arg^11^)CCMSH showed favorable tumor imaging properties in mice bearing murine melanoma (11). To improve the tumor/kidney uptake ratio and stability, a rhenium-cyclized α-MSH analog, Re-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_ (Re-CCMSH(Arg^11^)), was conjugated with DOTA. DOTA-Re-CCMSH(Arg^11^) was radiolabeled with ^64^Cu as a potential molecular imaging agent to target melanoma (12). ^64^Cu is a positron emitter with a physical half-life of 12.7 h and is suitable for PET imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+and+synthesis)]

McQuade et al. (13) reported the synthesis of ^64^Cu-DOTA-ReCCMSH(Arg^11^). The DOTA-CCMSH(Arg^11^) peptide was synthesized using standard Fmoc/HBTU(2-[1H-benzotriazole-1-yl]-l,1,3,3,-tetramethyluronium hexafluorophosphate) chemistry on an amide resin with a peptide synthesizer as reported previously by Chen et al. (10). A mixture of DOTA-CCMSH(Arg^11^) and ReOCl_3_ (1:1.5 molar ratio) was incubated for 2 h at 75°C. The cyclized peptide, DOTA-ReCCMSH(Arg^11^), was purified with high-performance liquid chromatography (HPLC). For ^64^Cu labeling, a solution of ^64^CuCl_3_ and DOTA-ReCCMSH(Arg^11^) in 0.1 M sodium acetate was heated for 60 min at 65ºC. Radiochemical purity (as confirmed with HPLC) was >95% with a specific activity of 11.1 GBq/mg (0.3 Ci/mg). better if it is per mole!

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+AND+in+vitro)]

Chen et al. (10) determined the 50% inhibition concentration (IC_50_) value of DOTA-ReCCMSH to be 1.2 ± 0.3 nM using B16/F1 murine melanoma cells. In comparison, the IC_50_ value of ReCCMSH was 2.9 ± 0.3 nM. Wei et al. (13) found that the IC_50_ value was 6.9 nM for Cu-DOTA-ReCCMSH. The radioactive ligand was ^125^I-Tyr^2^-[Nle^4^,D-Phe^7^]α-MSH.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+rodentia)]

McQuade et al. (13) performed biodistribution studies in female C57BL/6 mice (n = 5/group) bearing 10-day-old B16/F1 murine melanoma tumors. Each mouse received 0.2 MBq (0.005 mCi (8.3 pmol)) ^64^Cu-DOTA-ReCCMSH(Arg^11^). The radioactivity levels in percent injected dose per gram (% ID/g) were obtained at 30 min, 2 h, 4 h, and 24 h after injection, with tumor uptake values of 8.45 ± 1.42, 7.09 ± 3.20, 7.37 ± 1.26, and 4.01 ± 0.77, respectively. Tumor retention was high. Pre-administration of 10 nmol CBTE2A-ReCCMSH(Arg^11^) significantly reduced the tumor uptake to 0.99 ± 0.15% ID/g (P < 0.005) at 2 h after injection. No other tissues exhibited significant inhibition by CBTE2A-ReCCMSH(Arg^11^). The nontarget tissue uptake of ^64^Cu-CBTE2A-ReCCMSH(Arg^11^) was high at 30 min. However, the radioactivity was quickly cleared from all tissues at 2 h after injection (e.g., kidney: 12.71 ± 1.50% ID/g at 30 min and 8.57 ± 2.51% ID/g at 2 h; lung: 3.29 ± 1.16% ID/g at 30 min and 0.53 ± 0.06% ID/g at 2 h; blood: 2.95 ± 1.11% ID/g at 30 min and 0.19 ± 0.04% ID/g at 2 h; liver: 2.37 ± 0.28% ID/g at 30 min and 1.57 ± 0.42% ID/g at 2 h). The fast clearance from normal tissues and high tumor retention resulted in good tumor/nontarget tissue ratios at 2 h (e.g., tumor/muscle ratio of 44). When 15 mg D-lysine was coinjected with ^64^Cu-CBTE2A-ReCCMSH(Arg^11^), the kidney and tumor radioactivity levels were decreased by >60% at 2 h after injection. In contrast, the radioactivity levels in other major tissues were not affected. PET imaging of mice bearing the B16/F1 melanomas in the neck was conducted with intravenous injection of 5.55 MBq (0.15 mCi (0.25 nmol)) ^64^Cu-CBTE2A-ReCCMSH(Arg^11^) at 0.5, 2, 4, and 24 h. At 0.5 h, the tumor, kidney, blood, lung, and heart were visible. As the background radioactivity decreased, only the tumor, kidney, liver, and bladder were clearly visible by 2 h. Pre-injection of 10 nmol CBTE2A-ReCCMSH(Arg^11^) inhibited the tumor accumulation of radioactivity by ~80% at all time points, whereas there was little effect on the kidney and liver radioactivity levels.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+AND+human)]

No publication is currently available.

## NIH Support

R24 CA86307, P50 CA103130, R24 CA86060, P30 CA91842

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
4 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
5 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
6 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
7 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
8 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
9 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
10 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
11 Miao Y., Benwell K., Quinn T.P. (2007). 99mTc- and 111In-labeled alpha-melanocyte-stimulating hormone peptides as imaging probes for primary and pulmonary metastatic melanoma detection. J Nucl Med.
12 Wei L., Butcher C., Miao Y., Gallazzi F., Quinn T.P., Welch M.J., Lewis J.S. (2007). Synthesis and biologic evaluation of 64Cu-labeled rhenium-cyclized alpha-MSH peptide analog using a cross-bridged cyclam chelator. J Nucl Med.
13 McQuade P., Miao Y., Yoo J., Quinn T.P., Welch M.J., Lewis J.S. (2005). Imaging of melanoma using 64Cu- and 86Y-DOTA-ReCCMSH(Arg11), a cyclized peptide analogue of alpha-MSH. J Med Chem.